# AlexaFluor 700–Labeled regioselectively addressable functionalized template-[cyclo-(Arg-Gly-Asp-d-Phe-Lys)]_4_

Chemical name: | AlexaFluor 700–Labeled regioselectively addressable functionalized template-[cyclo-(Arg-Gly-Asp-d-Phe-Lys)]_4_
Abbreviated name: | A700-RAFT-RGD
Synonym: | A700-RAFT-c(-RGDfK-)_4_
Agent Category: | Peptides
Target: | Integrin α_v_β_3_
Target Category: | Receptors
Method of detection: | Optical imaging
Source of signal / contrast: | AlexaFluor 700
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=molecular%20imaging%20and%20integrin%20%CE%B1v%CE%B23)]

AlexaFluor 700 (A700)–Labeled regioselectively addressable functionalized template (RAFT)-[cyclo-(Arg-Gly-Asp-d-Phe-Lys)]_4_, abbreviated as A700-RAFT-RGD, is a tetrameric Arg-Gly-Asp (RGD)-based peptide conjugate synthesized by Briat et al. for tumor imaging by targeting integrin α_v_β_3_ (1).

Angiogenesis is a process of neovascular development and growth from preexisting vessels. Different from the normal blood vessel system, the neovasculature is chaotic and irregular in tumors with abnormal expression of diverse vascular surface biomarkers. These biomarkers have fewer kinetic compartments that must be crossed for intravenously administered agents to reach them (2, 3). Integrin α_v_β_3_ is one of these biomarkers, and it has been intensively investigated as a target for imaging and antiangiogenic therapy. Integrin α_v_β_3_ is minimally expressed in normal blood vessels but is significantly overexpressed in newly sprouting vasculature in tumors (4, 5). Small peptides are one group of ligands frequently used for targeting purposes, such as RGD, Asp-Gly-Arg, His-Gly-Phe, and Arg-Arg-Leu (3). The RGD tripeptide sequence is an adhesive protein recognition site, presenting in the extracellular matrix and blood. Integrin α_v_β_3_ binds extracellular matrix proteins through the exposed RGD tripeptide sequence. In general, RGD peptides are less selective (binding with 8 of the 24 integrins), degrade rapidly in vivo, and have a relatively low binding affinity (3, 6).

Development of multivalent RGD peptides is one approach to improve their properties. Boturyn et al. synthesized a RAFT-RGD platform based on a cyclic decapeptide scaffold that incorporates and presents in a spatially controlled manner two independent functional domains: a clustered ligand domain for integrin recognition and cell targeting, and a labeling domain for detection and characterization of this binding (7). This platform has been labeled with Cy5, ^99m^Tc, and ^64^Cu and has been shown to efficiently accumulate in tumors in animal models (8-11). Although the results are promising, approximately 30%–50% of the total dose of the labeled RAFT-RGD has been found to remain trapped in the kidneys several days after injection, which is at least partially due to the tetramerization of RGD peptides (8, 12, 13). Although peptides can be reabsorbed, endocytosed, and degraded by the lysosomes of proximal tubular cells, radiometal-chelated amino acids may be retained in the tubular cells, leading to radiation-induced toxicity and a weak imaging contrast for tumors surrounding the kidneys.

To reduce the renal accumulation of fluorescent and radiolabeled RAFT-RGD, Briat et al. evaluated the effect of Gelofusine on the renal reabsorption of these agents (1). Gelofusine is a gelatin-based plasma expander that consists of succinylated bovine gelatin molecules, a mixture of collagen-derived peptides. Infusion of Gelofusine has been reported to increase the renal excretion of megalin ligands and to decrease the retention of radiolabeled compounds in the cortical proximal tubules (14-16). The results by Briat et al. showed that Gelofusine significantly reduced the renal retention of labeled RAFT-RGD, while it increased the ratio of tumor to healthy tissue (1). The data obtained with ^111^In-DOTA-RAFT-RGD were summarized in the chapter on ^111^In-DOTA-RAFT-RGD in MICAD. This chapter summarizes the data obtained with A700-RAFT-RGD and Gelofusine.

### Related Resource Links:

Integrin α_v_β_3_-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Integrin%20%CE%B1v%CE%B23%20%20AND%20micad%5bbook%5d)

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=integrin%20%CE%B1v%CE%B23) and protein (http://www.ncbi.nlm.nih.gov/protein?term=integrin%20%CE%B1v%CE%B23) sequences of integrin α_v_β_3_

Articles on integrin α_v_β_3_ (http://www.ncbi.nlm.nih.gov/omim/?term=integrin) in Online Mendelian Inheritance in Man

Integrin α_v_β_3_-related clinical trials (http://clinicaltrials.gov/ct2/results?term=integrin+%CE%B1v%CE%B23) in ClinicTrials.gov

Reference sequences of integrin members (http://www.ncbi.nlm.nih.gov/gene?term=integrin) in RefSeq

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=RAFT-RGD%20and%20imaging)]

Boturyn et al. described the synthesis of the series of RAFT-RGD compounds (7). Briat et al. labeled RAFT-RGD with fluorescent A700 mono-N-hydroxysuccinimide ester by grafting the dye at a lysine side chain (1). The labeling efficiency was not reported nor was the A700 per RGD.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/19111043)]

Boturyn et al. characterized the series of RAFT-RGD compounds and their cellular internalization (7). No data are available for the binding and cellular internalization of A700-RAFT-RGD.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=RAFT-RGD%20and%20imaging)]

Ahmadi et al. and Briat et al. investigated the biodistribution of ^111^In-DOTA-RAFT-RGD in α_v_β_3_-positive mice bearing TS/A-pc (murine mammary carcinoma cells) tumors (1, 13). Briat et al. also analyzed the distribution of A700-RAFT-RGD, which showed results similar to the distribution of ^111^In-DOTA-RAFT-RGD (no detailed data provided) (1).

Briat et al. further studied the effects of Gelofusine on the biodistribution of A700-RAFT-RGD in mice bearing TS/A-pc tumors (n = 6 mice/group) (Table 1) (1). Each mouse received a tail vein injection of 200 µl (10 nmol dye/mouse) A700-RAFT-RGD. Gelofusine (4%) or phosphate-buffed saline (PBS) was preinjected 2–5 min before A700-RAFT-RGD injection. Fluorescent imaging was performed at 1 h and 24 h after injection, and the mice were then euthanized. Compared with PBS, preinjection of Gelofusine reduced the kidney uptake of A700-RAFT-RGD by 63% as measured from the dissected kidneys and by 31% as measured with noninvasive optical imaging (P < 0.01). The tumor uptake was not significantly affected by Gelofusine (P > 0.05). No blocking studies were reported.

Table 1: Effect of Gelofusine on the biodistribution of A700-RAFT-RGD.

| PBS | | | Gelofusine
Ratio | 1 h | 24 h | Dissected^1^ | 1 h | 24 h | Dissected^1^
T/M | 2.02 ± 0.09 | 2.18 ± 0.33 | 6.87 ± 0.34 | 1.95 ± 0.43 | 2.03 ± 0.64 | 3.80 ± 0.04
T/K | 0.66 ± 0.13 | 1.33 ± 0.01 | 0.35 ± 0.12 | 1.24 ± 0.26 | 1.68 ± 0.37 | 0.73 ± 0.41
Kidney^2^ | 10,457 ± 1,470 | 985 ± 213 | 4,601 ± 1,086 | 5,040 ± 580 | 682 ± 167 | 1,698 ± 61

^1^Data were obtained from dissected organs at 24 h after injection. Other data in the table were obtained directly from the images.

^2^Data are expressed as the mean of the relative light unit per pixel.

Abbreviations: T/M = tumor/muscle ratio; T/K = tumor/kidney ratio.

Confocal microscopy of the tissue sections of the dissected kidneys showed that A700-RAFT-RGD was mainly trapped in the renal cortex at 24 h after injection (1). There was no effect of Gelofusine on the A700-RAFT-RGD localization into the kidneys or into a particular cell type.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Briat A., Wenk C.H., Ahmadi M., Claron M., Boturyn D., Josserand V., Dumy P., Fagret D., Coll J.L., Ghezzi C., Sancey L., Vuillez J.P. (2012). Reduction of renal uptake of (111) In-DOTA-labeled and A700-labeled RAFT-RGD during integrin alpha(v) beta(3) targeting using single photon emission computed tomography and optical imaging. Cancer Sci.
2 Cai W., Chen X. (2008). Multimodality molecular imaging of tumor angiogenesis. J Nucl Med.
3 Lu X., Wang R.F. (2012). A concise review of current radiopharmaceuticals in tumor angiogenesis imaging. Curr Pharm Des.
4 Beer A.J., Schwaiger M. (2008). Imaging of integrin alphavbeta3 expression. Cancer Metastasis Rev.
5 Gaertner, F.C.,Schwaiger, M., and Beer, A.J. Molecular imaging of avb3 expression in cancer patients. Q J Nucl Med Mol Imaging. 2010
6 Turkbey B., Kobayashi H., Ogawa M., Bernardo M., Choyke P.L. (2009). Imaging of tumor angiogenesis: functional or targeted?. AJR Am J Roentgenol.
7 Boturyn D., Coll J.L., Garanger E., Favrot M.C., Dumy P. (2004). Template assembled cyclopeptides as multimeric system for integrin targeting and endocytosis. J Am Chem Soc.
8 Jin Z.H., Josserand V., Razkin J., Garanger E., Boturyn D., Favrot M.C., Dumy P., Coll J.L. (2006). Noninvasive optical imaging of ovarian metastases using Cy5-labeled RAFT-c(-RGDfK-)4. Mol Imaging.
9 Jin Z.H., Josserand V., Foillard S., Boturyn D., Dumy P., Favrot M.C., Coll J.L. (2007). In vivo optical imaging of integrin alphaV-beta3 in mice using multivalent or monovalent cRGD targeting vectors. Mol Cancer.
10 Sancey L., Ardisson V., Riou L.M., Ahmadi M., Marti-Batlle D., Boturyn D., Dumy P., Fagret D., Ghezzi C., Vuillez J.P. (2007). In vivo imaging of tumour angiogenesis in mice with the alpha(v)beta (3) integrin-targeted tracer 99mTc-RAFT-RGD. Eur J Nucl Med Mol Imaging.
11 Garanger E., Boturyn D., Jin Z., Dumy P., Favrot M.C., Coll J.L. (2005). New multifunctional molecular conjugate vector for targeting, imaging, and therapy of tumors. Mol Ther.
12 Cheng, K.T.,Garanger, E.,Josserand, V.,Jin, Z.,Foillard, S.,Boturyn, D.,Favrot, P.M.C.,Dumy, P., and Coll, J.L. Cy5-Regioselectively addressable functionalized template-[cyclo-(RGD-d-Phe-Lys)]4 peptide. 2004
13 Ahmadi M., Sancey L., Briat A., Riou L., Boturyn D., Dumy P., Fagret D., Ghezzi C., Vuillez J.P. (2008). Chemical and biological evaluations of an (111)in-labeled RGD-peptide targeting integrin alpha(V) beta(3) in a preclinical tumor model. Cancer Biother Radiopharm.
14 Vegt E., Wetzels J.F., Russel F.G., Masereeuw R., Boerman O.C., van Eerd J.E., Corstens F.H., Oyen W.J. (2006). Renal uptake of radiolabeled octreotide in human subjects is efficiently inhibited by succinylated gelatin. J Nucl Med.
15 van Eerd J.E., Vegt E., Wetzels J.F., Russel F.G., Masereeuw R., Corstens F.H., Oyen W.J., Boerman O.C. (2006). Gelatin-based plasma expander effectively reduces renal uptake of 111In-octreotide in mice and rats. J Nucl Med.
16 ten Dam M.A., Branten A.J., Klasen I.S., Wetzels J.F. (2001). The gelatin-derived plasma substitute Gelofusine causes low-molecular-weight proteinuria by decreasing tubular protein reabsorption. J Crit Care.